# [^18^F]3-(1H-Imidazol-4-yl)propyl-4-fluorobenzyl ether

Chemical name: | [^18^F]3-(1H-Imidazol-4-yl)propyl-4-fluorobenzyl ether
Abbreviated name: | [^18^F]Fluoroproxyfan
Synonym:
Agent Category: | Compound
Target: | Histamine H_3_ receptor
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Fluoroproxyfan)]

Histamine is a major neurotransmitter that plays important physiological roles (1, 2). There are four histamine receptor subtypes (H_1_ to H_4_) (3). Histamine H_3_ receptors (H_3_Rs) are presynaptic autoreceptors that negatively regulate the release of histamine and other neurotransmitters such as norepinephrine, GABA, dopamine, and acetylcholine in the central nervous system (CNS) (4). Consistent with the widespread projection of histaminergic neurons from the lateral hypothalamus, H_3_Rs are widely distributed in the CNS with high densities in the basal ganglia and are believed to play a variety of physiological roles, including regulation of feeding, arousal, cognition, pain, and endocrine systems (5-7). The H_3_Rs are also found in a wide variety of peripheral tissues (4). The H_3_Rs are GTP-binding-protein (G-protein)–coupled receptors that decrease Ca^2+^ influx into the cell and inhibit adenylyl cyclase.

Positron emission tomography (PET) and single-photon emission tomography of radioligands targeting histamine receptors allow visualization and analysis of histamine receptors in the human brain (8-10). [^11^C]Doxepin was synthesized and developed as a specific PET imaging agent for H_1_ receptors, showing strong and specific signals in the human brain (11). 3-(1H-Imidazol-4-yl)propyl-4-fluorobenzyl ether (fluoroproxyfan) was found to be a potent and selective H_3_R antagonist (10). [^18^F]Fluoroproxyfan was synthesized and evaluated as a specific PET imaging tool for H_3_Rs (12).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fluoroproxyfan%20and%20synthesis)]

Funaki et al. (12) reported a multi-step synthesis of [^18^F]fluoroproxyfan. First, [^18^F]fluorobenzyl alcohol was synthesized via nucleophilic substitution of 4-trimethylammonium benzaldehyde with K[^18^F]F/Kryptofix 2.2.2. Second, [^18^F]fluorobenzyl alcohol was reacted with Ph_3_Br_2_ to form [^18^F]fluorobenzyl bromide. Third, 3-(1-triphenylmethyl-1H-imidazol-4-yl)propanol was alkylated with [^18^F]fluorobenzyl bromide in the presence of silver triflate and 2,6-di-tert-butylpyridine, followed by acidic hydrolysis. [^18^F]Fluoroproxyfan was purified with high-performance liquid chromatography with a radiochemical yield of 8–11% (decay-corrected) on the basis of [^18^F]fluorobenzyl bromide and a specific activity of 412 GBq/μmol (11.1 Ci/μmol) at the end of synthesis. The total synthesis time was 90 min from the end of bombardment.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fluoroproxyfan%20and%20in%20vitro)]

In vitro binding of [^18^F]fluoroproxyfan was studied in rat brain tissue membranes (12). Binding of [^18^F]fluoroproxyfan was highest in the striatum, midbrain, cortex, hippocampus, and thalamus (~2.2–2.7 fmol/mg tissue), followed by the hypothalamus and brainstem (~1.5–1.7 fmol/mg tissue), whereas the lowest binding was in the cerebellum (~0.5 fmol/mg tissue). In vitro autoradiography studies of rat brain slices indicated selective binding of [^18^F]fluoroproxyfan to the striatum, thalamus, and cortex, and the accumulation of radioactivity was markedly reduced by co-incubation with fluoroproxyfan.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fluoroproxyfan%20and%20rodentia)]

Funaki et al. (12) performed in vivo biodistribution studies in normal rats injected intravenously with of 1.30-.1.85 MBq (0.035-0.050 mCi) [^18^F]fluoroproxyfan at 5–120 min. Results showed that the regional distribution of [^18^F]fluoroproxyfan was heterogeneous in the rat brain; it was especially higher in the thalamus, hypothalamus, and midbrain 60 min after injection. The thalamus/cerebellum and hypothalamus/cerebellum ratios were 1.7 ± 0.1 and 1.6 ± 0.3, respectively. Pretreatment with fluoroproxyfan (0.5 mg/kg) 15 min before [^18^F]fluoroproxyfan injection decreased the ratios to unity. Injection of fluoroproxyfan 30 min after the injection of [^18^F]fluoroproxyfan decreased the ratios with increasing doses of fluoroproxyfan, whereas no significant inhibition was observed in the cortex/cerebellum ratio. The peripheral organ with the highest accumulation was the lung, followed by the kidney, liver, small intestine, heart, and urinary bladder at 60 min. In the brain, >94% and >69% of [^18^F]fluoroproxyfan radioactivity remained intact at 30 and 120 min, respectively. However, one polar metabolite was found in the brain samples. On the other hand, the amounts of intact [^18^F]fluoroproxyfan in the plasma were 43% at 30 min and 20% at 120 min. Two polar metabolites were observed in the plasma samples.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fluoroproxyfan%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fluoroproxyfan%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fluoroproxyfan%20and%20human)]

No publication is currently available.

## References

1 Bongers G., Bakker R.A., Leurs R. (2007). Molecular aspects of the histamine H3 receptor. Biochem Pharmacol.
2 Brown R.E., Stevens D.R., Haas H.L. (2001). The physiology of brain histamine. Prog Neurobiol.
3 Hough L.B. (2001). Genomics meets histamine receptors: new subtypes, new receptors. Mol Pharmacol.
4 Leurs R., Bakker R.A., Timmerman H., de Esch I.J. (2005). The histamine H3 receptor: from gene cloning to H3 receptor drugs. Nat Rev Drug Discov.
5 Hancock A.A., Fox G.B. (2004). Perspectives on cognitive domains, H3 receptor ligands and neurological disease. Expert Opin Investig Drugs.
6 Ito C. (2004). The role of the central histaminergic system on schizophrenia. Drug News Perspect.
7 Passani M.B., Lin J.S., Hancock A., Crochet S., Blandina P. (2004). The histamine H3 receptor as a novel therapeutic target for cognitive and sleep disorders. Trends Pharmacol Sci.
8 Yanai K., Watanabe T., Yokoyama H., Meguro K., Hatazawa J., Itoh M., Iwata R., Ishiwata K., Takahashi T., Ido T. (1992). Histamine H1 receptors in human brain visualized in vivo by [11C]doxepin and positron emission tomography. Neurosci Lett.
9 Yanai K., Watanabe T., Hatazawa J., Itoh M., Nunoki K., Hatano K., Iwata R., Ishiwata K., Ido T., Matsuzawa T. (1990). Visualization of histamine H1 receptors in dog brain by positron emission tomography. Neurosci Lett.
10 Stark H., Purand K., Huls A., Ligneau X., Garbarg M., Schwartz J.C., Schunack W. (1996). [125I]iodoproxyfan and related compounds: a reversible radioligand and novel classes of antagonists with high affinity and selectivity for the histamine H3 receptor. J Med Chem.
11 Higuchi M., Yanai K., Okamura N., Meguro K., Arai H., Itoh M., Iwata R., Ido T., Watanabe T., Sasaki H. (2000). Histamine H(1) receptors in patients with Alzheimer's disease assessed by positron emission tomography. Neuroscience.
12 Funaki Y., Sato K., Kato M., Ishikawa Y., Iwata R., Yanai K. (2007). Evaluation of the binding characteristics of [(18)F]fluoroproxyfan in the rat brain for in vivo visualization of histamine H(3) receptor. Nucl Med Biol.